# ^99m^Tc-Ethylenedicysteine-folate

Chemical name: | ^99m^Tc-Ethylenedicysteine-folate
Abbreviated name: | ^99m^Tc-EC-folate
Synonym:
Agent category: | Compound
Target: | Folate receptor
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-EC%5BAll%20Fields%5D%20AND%20folate%5BAll%20Fields%5D)]

Folic acid is a water-soluble B vitamin (1). It is essential for methylation and DNA synthesis. The primary pathway for entry of folate into cells is through facilitated transporter, which has a low affinity for folate with K_m_ of 1-5 μM. Some cells in choroid plexus, kidney, lung, thyroid, spleen, placenta, and thymus also possess a higher affinity (K_d_, 0.5 nM) receptor that allows folate uptake via receptor-mediated endocytosis. Some human epithelial tumor cells were found to overexpress folate receptors (2). More than 90% of human ovarian and endometrial cancers express the high-affinity receptor, which is absent in the normal tissues. Breast, colorectal, renal, and lung carcinomas also over-expressed the folate receptor but to a lesser frequency (20-50%). ^99m^Tc-EC-folate was synthesized and developed as a folate receptor imaging agent (3).

### Related Resource Links:

- Chapters in MICAD (Folate receptor (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=folate+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Folate receptor (http://www.ncbi.nlm.nih.gov/gene/2348))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Folate receptor (http://www.ncbi.nlm.nih.gov/omim/136430))
- Clinical trials (Folate receptors (http://www.clinicaltrials.gov/ct2/results?term=folate+receptor))
- Drug information in FDA (Folate receptor (http://google2.fda.gov/search?q=folate+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-EC%5BAll%20Fields%5D%20AND%20%28folate%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D%29)]

L, L-Ethylenedicysteine (EC) was conjugated to folate-NH_2_ using sulfo-N-hydroxysulfosuccinimide (3). One EC (M.W. 268 Da) residue was estimated to conjugate to folate-NH_2_ (M.W. 483 Da) to form EC-folate. ^99m^Tc was complexed efficiently to EC-Folate to form ^99m^Tc-EC-folate with a radiochemical purity of >95%. The specific activity was calculated to be about 10 μCi/μg (0.37 MBq/μg) before in vivo injection to rats.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-EC%5bAll%20Fields%5d%20AND%20folate%20and%20in%20vitro)]

^99m^Tc-EC-folate was found to be stable at dog serum samples at 37ºC up to 4 h (3).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-EC%5BAll%20Fields%5D%20AND%20folate%20and%20rodentia)]

Rats were inoculated with rat mammary tumor cells, followed by intravenous injection (10 μCi/rat, 0.37 MBq/rat, 10 μg/rat) of ^99m^Tc-EC-folate or ^99m^Tc-EC 14 -17 days after tumor transplantation (3). Tumor-to-blood uptake ratios for ^99m^Tc-EC-folate rats increased as a function of time, whereas these ratios decreased for ^99m^Tc-EC in the same period. Tumor uptake in ^99m^Tc-EC-folate rats was about 1-fold higher than ^99m^Tc-EC rats. The kidneys and liver were the organs with high uptakes of both tracers. Both tracers were excreted mainly in the urine. Co-injections of rats with 0.15 mol/kg of unlabeled folate blocked the uptake of ^99m^Tc-EC-folate by 30%.

Scintigraphic images of rats given ^99m^Tc-EC-folate (0.5 mCi/rat, 18.5 MBq/rat, 50 μg/rat) showed that tumors in the right hind legs could be well visualized at 1-4 h (3). ^99m^Tc-EC-folate could be a useful tool for imaging folate receptor positive tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-EC%5BAll%20Fields%5D%20AND%20folate%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-EC%5BAll%20Fields%5D%20AND%20folate%20and%20%28primates%20not%20humans%29)]

No publication is currently available

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-EC%5BAll%20Fields%5D%20AND%20folate%20and%20humans)]

No publication is currently available.

## NIH Support

CA-16672

## References

1 Stanger O. (2002). Physiology of folic acid in health and disease. Curr Drug Metab.
2 Ke C. Y., Mathias C. J., Green M. A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
3 Ilgan S., Yang D. J., Higuchi T., Zareneyrizi F., Bayhan H., Yu D., Kim E. E., Podoloff D. A. (1998). 99mTc-ethylenedicysteine-folate: a new tumor imaging agent. Synthesis, labeling and evaluation in animals. Cancer Biother Radiopharm.